# ^99m^Tc-Hydrazinonicotinamide-annexin V

Chemical name: | ^99m^Tc-Hydrazinonicotinamide-annexin V
Abbreviated name: | ^99m^Tc-HYNIC-annexin V
Synonym:
Agent Category: | Protein
Target: | Phosphatidylserine
Target Category: | Binding
Method of detection: | SPECT, planar
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=468888), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4809273) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=308) for more information about annexin V.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mtc%20hynic%20annexin%20V)]

Apoptosis, or programmed cell death, plays an important role in the pathophysiology of many diseases, such as cancer, neurodegenerative disorders, vascular disorders, and chronic hepatitis, as well as in the biology of normal cells, such as epithelial cells and immune cells (1). Apoptosis is gene regulated (2) and involves the proteolysis of intracellular components by activation of a series of proteolytic enzymes, called caspases, and changes of plasma membrane structure by translocase, floppase, and scramblase (3-5). As a result, there is rapid redistribution of phosphatidylserine (PS) from the inner membrane leaflet to the outer membrane leaflet of apoptotic cells, exposing the anionic head group of PS. On the other hand, PS is also accessible for annexin V binding in necrotic cells because of disruption of the plasma membrane.

Annexin V is a 36-kDa endogenous human protein that is produced by the epithelial cells of many tissues, such as placenta, umbilical vessels, liver, spleen, kidney, heart, uterus, and skeletal muscle, as well as by erythrocytes, leukocytes, endothelial cells, and platelets (6). Annexin V binds to PS with high affinity (K_d_ = 7 nM) with 8 annexin V molecules per PS molecule (3, 7, 8). Apoptosis can be induced by chemicals, radiation, cytokines, hormones, and various pathologic conditions (5); therefore, the ability to monitor apoptosis in association with disease progression or regression should provide important information for clinical applications. Annexin V has been radiolabeled with ^123^I, ^125^I, and ^99m^Tc for single-photon emission computed tomography (SPECT) imaging (9, 10), and hydrazinonicotinamide (HYNIC) has been conjugated to human recombinant annexin V to form HYNIC-annexin V (11). ^99m^Tc-HYNIC-annexin V is being developed as an imaging agent to study apoptotic and necrotic cells in humans.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mtc%20hynic%20annexin%20V%20and%20synthesis)]

In the method described by Blankenberg et al. (11), HYNIC was conjugated to human recombinant annexin V to form HYNIC-annexin V by use of succinimidyl 6-HYNIC. HYNIC-annexin V was purified by dialysis with a yield of >94%, and the ratio of HYNIC to annexin V was 0.9:1. A mixture of HYNIC-annexin V (100 μg) and [^99m^Tc]pertechnetate (148-740 MBq (4-20 mCi)) was reacted in a solution containing tricine/SnCl_2_ at room temperature for 60 min. ^99m^Tc-HYNIC-annexin V was purified by column chromatography to give a yield of 56%, with a radiochemical purity >97% and a specific activity >1.95 MBq/μg of protein (50 μCi/μg of protein). Verbeke et al. (12) reported optimized preparation of ^99m^Tc-HYNIC-annexin V with 95% labeling yields by reaction of 60-90 μg of HYNIC-annexin V, 0.37-1.11 GBq (10-30 mCi) of ^99m^TcO_4_^-^, 10-20 μg of SnCl_2_·2 H_2_O, and 1.5 mg of tricine.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mtc%20hynic%20annexin%20V%20and%20in%20vitro)]

^99m^Tc-HYNIC-annexin V has been shown to selectively bind to apoptotic Jurkat T cells (induced by serum deprivation, doxorubicin, and anti-FAS antibody) and thymocytes (induced by dexamethasone) (13). The increases in ^99m^Tc-HYNIC-annexin V radioactivity were correlated with fluorescein isothiocyanate (FITC)-annexin V fluorescence intensities as measured by flow cytometry. The IC_50_ values of annexin V, HYNIC-annexin V, and decayed ^99m^Tc-HYNIC-annexin V for inhibition of FITC-annexin V binding to PS were 8, 10.5, and 12.3 nM, respectively. There thus was only a minimal loss of binding affinity by the modified annexin V.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mtc%20hynic%20annexin%20V%20and%20rodentia)]

Blankenberg et al. (11, 13) performed biodistribution studies in normal mice. Their results indicated high accumulation of radioactivity in the kidney (187% of injected dose (ID)/g of tissue), followed by the spleen (17% ID/g), liver (15% ID/g), stomach (5% ID/g), and lung (3% ID/g) at 60 min after injection of 0.74-1.85 MBq (0.02-0.05 mCi) of ^99m^Tc-HYNIC-annexin V. The radioactivity levels in the brain, heart, and thymus were the lowest (<0.2% ID/g), and the radioactivity in the blood was 2%. There was a 3-fold increase in hepatic accumulation of ^99m^Tc-HYNIC-annexin V in mice treated with anti-FAS antibody to induce apoptosis in the liver compared with control mice. Accumulation of ^99m^Tc-human serum albumin in both the kidney and liver was similar in the FAS-treated and control mice. There was also a 2- to 6-fold increase in ^99m^Tc-HYNIC-annexin V accumulation at apoptotic sites in mice bearing 38C13 B-cell lymphomas treated with cyclophosphamide and in rats with transplanted heterotopic cardiac allografts.

Blankenberg et al. (14) performed a ^99m^Tc-HYNIC-annexin V SPECT imaging study in cyclophosphamide-treated rats (8-10 weeks old); their results showed increased accumulation of radioactivity in the femur, pelvis, vertebrae, and spleen as early as 8 h after cyclophosphamide treatment (100 mg/kg). Older rats (5-6 months old) showed a slower response to cyclophosphamide treatment and delayed recovery of bone marrow and splenic tissues. Therefore, the immunosuppressive effect of cyclophosphamide can be visualized by SPECT imaging with ^99m^Tc-HYNIC-annexin V.

Using ^99m^Tc-HYNIC-annexin V SPECT, Takei et al. (15) studied the effects of chemotherapy with gemcitabine and cyclophosphamide in rats bearing allogenic hepatomas. After chemotherapy, the accumulation of ^99m^Tc-HYNIC-annexin V in the tumors increased significantly in the gemcitabine group (0.062% ID/g × kg) and in the cyclophosphamide group (0.050% ID/g × kg) compared with that in the control group (0.031% ID/g × kg; P < 0.01). In contrast, the uptake of 2-[^18^F]fluoro-2-deoxy-D-glucose ([^18^F]FDG) in the tumors decreased significantly in the gemcitabine and cyclophosphamide groups compared with the control group (P < 0.01). In addition, tumor uptake of [^18^F]FDG negatively correlated with ^99m^Tc-HYNIC-annexin V accumulation (r = -0.75; P < 0.01). In the gemcitabine and cyclophosphamide groups, the percentages of terminal deoxynucleotidyl transferase-mediated deoxyuridine triphosphate nick-end labeling (TUNEL)-positive cells were significantly higher (P < 0.01) than in the control group (10.2 ± 1.7, 8.0 ± 1.5, and 5.2 ± 1.5%, respectively), whereas glucose transporter-1 expression showed little change in histologic analyses. Hence, these data indicate that an enhanced apoptotic reaction correlated with suppressed tumor glucose utilization after cytotoxic chemotherapy as determined by radiotracers and histologic evaluation.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mtc%20hynic%20annexin%20V%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mtc%20hynic%20annexin%20V%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mtc%20hynic%20annexin%20V%20and%20human)]

Various SPECT studies using ^99m^Tc-HYNIC-annexin V have been performed in patients with head-and-neck carcinoma and showed that absolute uptake values in the primary tumors correlate well with the number of apoptotic cells as measured by the TUNEL assay or other histologic analyses (16-19). However, SPECT failed to identify most of the lymph node lesions detected by computed tomography, mainly because the lymph nodes are smaller in size than the primary tumors and contain mostly focal metastases.

In a study of 33 patients with lymphoma (n = 26) and other tumors, Kartachova et al. (20) concluded that partial or complete tumor response to therapy was associated with a marked increase in ^99m^Tc-HYNIC-annexin V in the tumors. In contrast, patients with stable or progressive disease showed low ^99m^Tc-HYNIC-annexin V accumulation before treatment and no increase after treatment. Therefore, ^99m^Tc-HYNIC-annexin V SPECT may be used to identify patients who would respond to therapies and to assess the effectiveness of therapies.

Kemerink et al. (21) reported on SPECT studies in 6 normal volunteers after injection of 250 MBq (6.8 mCi) of ^99m^Tc-HYNIC-annexin V. The kidneys received the highest dose of radioactivity (49.7% ID) at 3 h after injection, followed by the liver (13.1% ID), the red marrow (9.2% ID), and the spleen (4.6% ID). More than 90% of the blood activity was cleared rapidly with a half-life of 24 min. The radioactivity was excreted almost exclusively through the urine (22.5% ID at 24 h), and hardly any radioactivity was seen in the feces. Absorbed doses were 196 μGy/MBq (0.73 rad/mCi) for the kidneys, 41 μGy/MBq (0.15 rad/mCi) for the spleen, 16.9 μGy/MBq (0.063 rad/mCi) for the liver, and 8.4 μGy/MBq (0.031 rad/mCi) for the red marrow. The effective dose was 11.0 ± 0.8 μSv/MBq (40.7 ± 3.0 mrem/mCi).

## Human Studies

HL-47151, HL-61717

## References

1 Thompson C.B. (1995). Apoptosis in the pathogenesis and treatment of disease. Science.
2 Steller H. (1995). Mechanisms and genes of cellular suicide. Science.
3 Thiagarajan P., Tait J.F. (1990). Binding of annexin V/placental anticoagulant protein I to platelets. Evidence for phosphatidylserine exposure in the procoagulant response of activated platelets. J Biol Chem.
4 Song Z., Steller H. (1999). Death by design: mechanism and control of apoptosis. Trends Cell Biol.
5 Blankenberg F.G., Tait J., Ohtsuki K., Strauss H.W. (2000). Apoptosis: the importance of nuclear medicine. Nucl Med Commun.
6 Blankenberg F.G., Strauss H.W. (2001). Will imaging of apoptosis play a role in clinical care? A tale of mice and men. Apoptosis.
7 van Heerde W.L., de Groot P.G., Reutelingsperger C.P. (1995). The complexity of the phospholipid binding protein Annexin V. Thromb Haemost.
8 Tait J.F., Cerqueira M.D., Dewhurst T.A., Fujikawa K., Ritchie J.L., Stratton J.R. (1994). Evaluation of annexin V as a platelet-directed thrombus targeting agent. Thromb Res.
9 Blankenberg F.G. (2004). Recent advances in the imaging of programmed cell death. Curr Pharm Des.
10 Lahorte C., Slegers G., Philippe J., Van de Wiele C., Dierckx R.A. (2001). Synthesis and in vitro evaluation of 123I-labelled human recombinant annexin V. Biomol Eng.
11 Blankenberg F.G., Katsikis P.D., Tait J.F., Davis R.E., Naumovski L., Ohtsuki K., Kopiwoda S., Abrams M.J., Darkes M., Robbins R.C., Maecker H.T., Strauss H.W. (1998). In vivo detection and imaging of phosphatidylserine expression during programmed cell death. Proc Natl Acad Sci U S A.
12 Verbeke K., Kieffer D., Vanderheyden J.L., Reutelingsperger C., Steinmetz N., Green A., Verbruggen A. (2003). Optimization of the preparation of 99mTc-labeled Hynic-derivatized Annexin V for human use. Nucl Med Biol.
13 Blankenberg F.G., Katsikis P.D., Tait J.F., Davis R.E., Naumovski L., Ohtsuki K., Kopiwoda S., Abrams M.J., Strauss H.W. (1999). Imaging of apoptosis (programmed cell death) with 99mTc annexin V. J Nucl Med.
14 Blankenberg F.G., Naumovski L., Tait J.F., Post A.M., Strauss H.W. (2001). Imaging cyclophosphamide-induced intramedullary apoptosis in rats using 99mTc-radiolabeled annexin V. J Nucl Med.
15 Takei T., Kuge Y., Zhao S., Sato M., Strauss H.W., Blankenberg F.G., Tait J.F., Tamaki N. (2005). Enhanced apoptotic reaction correlates with suppressed tumor glucose utilization after cytotoxic chemotherapy: use of 99mTc-Annexin V, 18F-FDG, and histologic evaluation. J Nucl Med.
16 van de Wiele C., Lahorte C., Vermeersch H., Loose D., Mervillie K., Steinmetz N.D., Vanderheyden J.L., Cuvelier C.A., Slegers G., Dierck R.A. (2003). Quantitative tumor apoptosis imaging using technetium-99m-HYNIC annexin V single photon emission computed tomography. J Clin Oncol.
17 Vermeersch H., Ham H., Rottey S., Lahorte C., Corsetti F., Dierckx R., Steinmetz N., Van de Wiele C. (2004). Intraobserver, interobserver, and day-to-day reproducibility of quantitative 99mTc-HYNIC annexin-V imaging in head and neck carcinoma. Cancer Biother Radiopharm.
18 Vermeersch H., Loose D., Lahorte C., Mervillie K., Dierckx R., Steinmetz N., Vanderheyden J.L., Cuvelier C., Slegers G., Van de Wiele C. (2004). 99mTc-HYNIC Annexin-V imaging of primary head and neck carcinoma. Nucl Med Commun.
19 Vermeersch H., Mervillie K., Lahorte C., Loose D., Dierck R.A., Steinmetz N., Cuvelier C., Slegers G., Van de Wiele C. (2004). Relationship of 99mTc-HYNIC annexin V uptake to microvessel density, FasL and MMP-9 expression, and the number of tumour-infiltrating lymphocytes in head and neck carcinoma. Eur J Nucl Med Mol Imaging.
20 Kartachova M., Haas R.L., Olmos R.A., Hoebers F.J., van Zandwijk N., Verheij M. (2004). In vivo imaging of apoptosis by 99mTc-Annexin V scintigraphy: visual analysis in relation to treatment response. Radiother Oncol.
21 Kemerink G.J., Liu X., Kieffer D., Ceyssens S., Mortelmans L., Verbruggen A.M., Steinmetz N.D., Vanderheyden J.L., Green A.M., Verbeke K. (2003). Safety, biodistribution, and dosimetry of 99mTc-HYNIC-annexin V, a novel human recombinant annexin V for human application. J Nucl Med.